# ^125^I-Single-chain antibody B1 targeting a pancreatic β-cell surface antigen

Chemical name: | ^125^I-Single-chain antibody B1 targeting a pancreatic β-cell surface antigen
Abbreviated name: | ^125^I-SCA B1
Synonym:
Agent category: | Antibody
Target: | Pancreatic β-cell specific antigen
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^125^I
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=single-chain%20antibody%20pancreatic%20islets)]

The β-cell mass (BCM) is a useful indicator of the function of the pancreas. In type I diabetes, β-cells are destroyed, leading to a dramatic decrease in BCM. In type II diabetes, there is a slow and continuous decrease in BCM because of peripheral insulin resistance and increased demand for insulin. Vesicular monoamine transporter (VMAT2) is present in brain monoaminergic neurons and is responsible for collecting neurotransmitters (e.g., dopamine, norepinephrine, and serotonin) from the cytoplasm and storing them in vesicles for synaptic release (1). VMAT2 is also highly expressed by β-cells in the endocrine pancreas but not in the exocrine pancreas. VMAT2 is expressed mainly on the β-cells in the islets of Langerhans and comprises 1%–2% of the pancreatic mass. VMAT2 is a potential target for noninvasive assessment of BCM and pancreatic function. VMAT2 has been studied noninvasively in vivo with positron emission tomography (PET) using [^11^C]dihydrotetrabenazine (2-hydroxy-3-isobutyl-9-[^11^C]methoxy-10-methoxy-1,2,3,4,6,7-hexahydro-11bH-benzo[a]quinolizine, also known as [^11^C]DTBZ (http://www.ncbi.nlm.nih.gov/books/NBK23597/)) in the human brain and pancreas. However, a human clinical study showed that the high nonspecific binding in the exocrine pancreas may appear to overestimate BCM on pancreatic [^11^C]DTBZ PET scans (2). Glucagon-like peptide-1 receptor (GLP-1R) has been shown to be highly overexpressed in human insulinomas and gastrinomas and has been evaluated with various noninvasive imaging studies of β-cells (3-5). Other β-cell imaging probes have also been studied (6-8).

Brogren et al. (9) prepared a rat monoclonal autoantibody (IC2) with lymphocytes isolated from the spleen and lymph nodes of a spontaneously diabetic BB rat. IC2 is a rat IgM kappa monoclonal antibody. The binding of IC2 to β-cells is sensitive to protease treatments. IC2 shows little binding to other rat tissues; however, IC2 exhibits binding to mouse, hamster, and human β-cells (8). Moore et al. (10) showed ^111^In-diethylenetriamine pentaacetic acid-IC2 (^111^In-DTPA-IC2 (http://www.ncbi.nlm.nih.gov/books/NBK83903/)) binding to β-cells in normal mice and reduced binding to β-cells in mice treated with streptozotocin (STZ) to induce BCM loss and diabetes. However, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging (11). Smaller antibody fragments, such as single-chain antibody (SCA), Fab', or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys (12). SCA comprises a single polypeptide in which the V_H_ (variable heavy chain) and V_L_ (variable light chain) domains are attached to one another by a flexible linker. Using phage-display screening of human SCA library with a rat β-cell insulinoma INS-1 tumor cell line, Ueberberg et al. (13) identified SCA B1 to be β-cell-specific. ^125^I-SCA B1 has been evaluated as a potential imaging probe for β-cells.

### Related Resource Links:

- Chapters in MICAD (β-cells (http://www.ncbi.nlm.nih.gov/books?term=beta-cell%20AND%20micad%5Bbook%5D), GLP-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (VMAT2 (http://www.ncbi.nlm.nih.gov/gene/6571), GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VMAT2 (http://www.ncbi.nlm.nih.gov/omim/193001), GLP-1R (http://omim.org/entry/138032))
- Clinical trials (VMAT2 (http://www.clinicaltrials.gov/ct2/results?term=VMAT2), Exendin (http://www.clinicaltrials.gov/ct2/results?term=GLP-1))
- Drug information in FDA (VMAT2 (http://google2.fda.gov/search?q=VMAT2&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=10), Exendin (http://google2.fda.gov/search?q=exendin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=single-chain%20antibody%20pancreatic%20islets+synthesis)]

SCA B1 were labeled with ^125^I using the chloramine-T method as described previously (14). The radiochemical purity, specific activity, and labeling yield of ^125^I-SCA B1 were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=single-chain%20antibody%20pancreatic%20islets+in+vitro)]

Ueberberg et al. (13) performed in vitro indirect fluorescence staining with SCA B1 on excised human pancreatic islets (β-cells). SCA B1 co-localized with insulin-positive β-cells in the pancreatic islets with no binding to the glucagon-producing exocrine cells. ^125^I-SCA B1 showed rapid binding to INS-1 cells at 4ºC, with a binding half-life of 8.0 min. The binding was saturable with a binding constant (K_d_) of 4.1 µM and 7,023 binding sites/cell. The binding of ^125^I-SCA B1 to INS-1 cells was 514-fold higher than the binding to rat AR42J pancreatic exocrine cells. A maximum capacity of 650,307 ^125^I-SCA B1 molecules was estimated to be internalized per INS-1 cell after incubation at 37ºC. No effects of SCA B1 (doses of 0.13 and 0.5 nmol) were observed on cell viability and apoptosis of INS-1 cells after overnight incubation at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=single-chain%20antibody%20pancreatic%20islets+rodentia)]

Ex vivo biodistribution studies were performed in normal rats (n = 7) and rats pretreated for 14 d with low (n = 5) and high (n = 5) doses of streptozotocin (STZ) to induce diabetes (13). These studies were performed at 2 h after injection of 18.5 µBq (0.5 µCi) ^125^I-SCA B1. Pancreatic accumulation values were 0.5% injected dose/gram (ID/g), 0.2% ID/g, and 0.1% ID/g in the control, low-dose, and high-dose STZ rats, respectively. There was a linear correlation between pancreatic accumulation of radioactivity and BCM (r^2^ = 0.937). There was an inverse correlation between blood glucose levels and pancreatic accumulation of radioactivity (r^2^ = 0.876). The blood circulation half-life of ^125^I-SCA B1 in control rats was 22.7 min. Histoimmunostaining showed a co-localization of SCA B1 to the insulin-positive β-cells in the pancreatic islets with no binding to the glucagon-producing exocrine cells. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=single-chain%20antibody%20pancreatic%20islets+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=single-chain%20antibody%20pancreatic%20islets+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=single-chain%20antibody%20pancreatic%20islets+human)]

No publication is currently available.

## NIH support

DK072473

## References

1 Schuldiner S. (1994). A molecular glimpse of vesicular monoamine transporters. J Neurochem.
2 Goland R., Freeby M., Parsey R., Saisho Y., Kumar D., Simpson N., Hirsch J., Prince M., Maffei A., Mann J.J., Butler P.C., Van Heertum R., Leibel R.L., Ichise M., Harris P.E. (2009). 11C-dihydrotetrabenazine PET of the pancreas in subjects with long-standing type 1 diabetes and in healthy controls. J Nucl Med.
3 Brom M., Oyen W.J., Joosten L., Gotthardt M., Boerman O.C. (2010). 68Ga-labelled exendin-3, a new agent for the detection of insulinomas with PET. Eur J Nucl Med Mol Imaging.
4 Christ E., Wild D., Forrer F., Brandle M., Sahli R., Clerici T., Gloor B., Martius F., Maecke H., Reubi J.C. (2009). Glucagon-like peptide-1 receptor imaging for localization of insulinomas. J Clin Endocrinol Metab.
5 Reiner T., Thurber G., Gaglia J., Vinegoni C., Liew C.W., Upadhyay R., Kohler R.H., Li L., Kulkarni R.N., Benoist C., Mathis D., Weissleder R. (2011). Accurate measurement of pancreatic islet beta-cell mass using a second-generation fluorescent exendin-4 analog. Proc Natl Acad Sci U S A.
6 Malaisse W.J., Louchami K., Sener A. (2009). Noninvasive imaging of pancreatic beta cells. Nat Rev Endocrinol.
7 Moore A. (2009). Advances in beta-cell imaging. Eur J Radiol.
8 Saudek F., Brogren C.H., Manohar S. (2008). Imaging the Beta-cell mass: why and how. Rev Diabet Stud.
9 Brogren C.H., Hirsch F., Wood P., Druet P., Poussier P. (1986). Production and characterization of a monoclonal islet cell surface autoantibody from the BB rat. Diabetologia.
10 Moore A., Bonner-Weir S., Weissleder R. (2001). Noninvasive in vivo measurement of beta-cell mass in mouse model of diabetes. Diabetes.
11 Holliger P., Hudson P.J. (2005). Engineered antibody fragments and the rise of single domains. Nat Biotechnol.
12 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
13 Ueberberg S., Meier J.J., Waengler C., Schechinger W., Dietrich J.W., Tannapfel A., Schmitz I., Schirrmacher R., Koller M., Klein H.H., Schneider S. (2009). Generation of novel single-chain antibodies by phage-display technology to direct imaging agents highly selective to pancreatic beta- or alpha-cells in vivo. Diabetes.
14 Hampe C.S., Wallen A.R., Schlosser M., Ziegler M., Sweet I.R. (2005). Quantitative evaluation of a monoclonal antibody and its fragment as potential markers for pancreatic beta cell mass. Exp Clin Endocrinol Diabetes.